# ^99m^Tc-Labeled murine IgM monoclonal antibody, fanolesomab, that targets the CD15 glycoprotein antigen

Chemical name: | ^99m^Tc-Labeled murine IgM monoclonal antibody, fanolesomab, that targets the CD15 glycoprotein antigen
Abbreviated name: | ^99m^Tc-Fanolesomab
Synonym: | NeutroSpec^®^; LeuTech; anti–stage-specific embryonic antigen-1 (anti-SSEA-1) antibody; MCA-480
Agent Category: | Antibody
Target: | Cluster of differentiation 15 (CD15) glycoprotein
Target Category: | Antigen
Method of detection: | Single-photon emission computed tomography (SPECT); gamma planar imaging
Source of signal / contrast: | ^99m^Tc
Activation: | No
Studies: | - In vitro; - Humans | Structure not available in PubChem (http://pubchem.ncbi.nlm.nih.gov/).

## Background

[PubMed (http://www.ncbi.nlm.nih.gov/pubmed?term=99mTc-Fanolesomab&cmd=DetailsSearch)]

Infection is one of the most common causes of morbidity in patients, especially for those who have undergone invasive surgery, and nuclear tracers such as ^67^Ga-citrate and autologous leukocytes labeled with ^111^In-oxine- or ^99m^Tc-hexamethylpropyleneamine oxime (^111^In- or ^99m^Tc-HMPAO) are often used to localize the infection to initiate treatment (1, 2). However, these tracers have limitations. ^67^Ga-Citrate produces low-resolution images with a gamma camera and shows high accumulation in the liver, colon, genitals, and the urinary tract (2). To use ^111^In- or ^99m^Tc-labeled HMPAO, leukocytes from the patient have to be isolated, labeled ex vivo with the radiolabeled compounds, and reinfused into the patient to detect the infection with scintigraphy. This procedure has to be performed by a skilled technician, may not always be convenient, is time-consuming, and can be risky for the technician as well as the patient (2). Investigators have also used ^111^In- or ^99m^Tc-labeled human immunoglobulin or ^123^I-interleukin to detect infections, but these agents tend to accumulate in the interstitial spaces, have low uptake at the site of infection, and are not always able to distinguish between infections and inflammation (1). Radionuclide-labeled peptides such as ubiquicidin or its derivatives (3), P483H-^99m^Tc (4) and ^99m^Tc-P1827DS (5), have been used to detect infections under preclinical or clinical conditions, but none of these agents are approved by the United States Food and Drug Administration (FDA) as agents to detect infection.

Researchers have also evaluated several radiolabeled murine monoclonal antibodies (mAb) that target either the cluster of differentiation 67 (CD67) antigen or the CD15 antigen (e.g., anti–stage-specific embryonic antigen-1 (anti-SSEA-1), also known as fanolesomab) on neutrophils to detect infections in humans (for details, see Shanthly et al. (1)). However, the anti-CD67 mAbs had a low affinity for the target (K_d_ = 10−^8^ M) and required 24 h imaging to obtain proper diagnosis, and a high percentage of the patients developed antibodies against the mouse antibodies. ^99m^Tc-Sulesomab (LeukoScan (http://www.ema.europa.eu/ema/index.jsp?curl=pages/medicines/human/medicines/000111/human_med_000883.jsp&mid=WC0b01ac058001d124&murl=menus/medicines/medicines.jsp&jsenabled=true)), the Fab’ fragment of IMMU-MN3, a murine mAb, is approved in some European countries for the detection of infection and inflammation in the bones of patients with osteomyelitis (http://my.clevelandclinic.org/disorders/osteomyelitis/hic_osteomyelitis.aspx) (6). In 2004, ^99m^Tc-labeled fanolesomab (now known as NeutroSpec^®^ (http://dailymed.nlm.nih.gov/dailymed/lookup.cfm?setid=af67a2f3-65b7-4a6e-9a51-315a280f976b)) was approved by the FDA (http://www.accessdata.fda.gov/scripts/cder/drugsatfda/index.cfm?fuseaction=Search.DrugDetails&#totable) for use in the United States as a diagnostic radiopharmaceutical for scintigraphic imaging of patients (>5 years of age) exhibiting signs and symptoms of appendicitis (http://digestive.niddk.nih.gov/ddiseases/pubs/appendicitis/) (the clinical trial information is not available on the www.clinicaltrial.gov web site). This mAb binds to the 3-lactose-N-fucopentose carbohydrate that defines the CD15 antigen that is expressed on the surface of human neutrophils (1). In 2005, the marketing of ^99m^Tc-fanolesomab was suspended in the United States (http://www.fda.gov/Drugs/DrugSafety/PostmarketDrugSafetyInformationforPatientsandProviders/DrugSafetyInformationforHeathcareProfessionals/PublicHealthAdvisories/ucm051652.htm) because, postmarketing, two patients died and an additional 15 patients experienced life-threatening cardiopulmonary events immediately after receiving this radiochemical. The current marketing status of ^99m^Tc-fanolesomab is not clear.

### Related Resource Links

Cluster differentiation (CD) antigens in PubMed (http://www.ncbi.nlm.nih.gov/pubmed?term=Cluster%20differentiation%20antigens&cmd=DetailsSearch).

CD15 in PubMed (http://www.ncbi.nlm.nih.gov/pubmed?term=CD15).

CD15 in Online Mendelian Inheritance in Man Database (OMIM) (http://omim.org/entry/104230).

## Synthesis

[PubMed (http://www.ncbi.nlm.nih.gov/pubmed?term=99mTc-fanolesomab%20synthesis&cmd=DetailsSearch)]

The preparation of ^99m^Tc-fanolesomab from a freeze-dried kit that was commercially available in the United States has been described by Tronco et al. (7). Briefly, the mAb was supplied in a vial containing maltose monohydrate, sodium potassium tartrate tetrahydrate, succinic acid, stannous tartrate, glycine, and disodium edetate dihydrate. Before use, the contents of the vial were reconstituted with 0.2–0.35 mL ^99m^Tc-pertechnetate (740–1480 MBq (~2–4 mCi)), incubated at 37°C for 30 min, and the final volume was brought up to 1 mL with 500 mg/mL ascorbic acid. The final product had a radiochemical purity of >90% as determined with thin-layer chromatography. The specific activity of the labeled mAb was 5.5–7.4 GBq/0.66 μmol (135–200 mCi/μmol). The radiolabeled mAb was used within 6 h after synthesis.

Thakur et al. isolated anti-SSEA-1 mAb from a hybridoma cell line (MCA-480) and labeled it with ^99m^Tc using two different methods (8). For the first procedure, the mAb was conjugated with diethylenetriamine pentaacetic acid (DTPA) and then labeled with ^99m^Tc (8). In the second procedure, the anti-SSEA-1 mAb was labeled directly with the radionuclide. The radiochemical yields with the two procedures were reported to be 94.8 ± 1.4% and 95.8 ± 3.5%, respectively, and the amount of colloids in both preparations was <5%. The radiochemical purity and specific activities of the mAb labeled with the two procedures were not reported. The final product from both procedures was formulated in 0.9% sodium chloride containing 3.0% human serum albumin and sterilized by passing through a 0.22-micron filter. The R_f_ value of the labeled mAb on instant thin-layer chromatography was reported to be 1.0, and the R_f_ of the colloid fraction was 0.0 (8).

In another study (9), the anti-SSEA-1 mAb was labeled with ^99m^Tc after conjugation with DTPA (the DTPA:mAb ratio was determined to be 1), and the ^99m^Tc-labeled mAb had a radiochemical purity of at least 80% as determined with high-performance liquid chromatography. The radiochemical yield and specific activity of the final product were not reported.

## In Vitro Studies: Testing in Cells and Tissues

[PubMed (http://www.ncbi.nlm.nih.gov/pubmed/?term=%22SUBSTANCENAME%22%5BSubstance%20Name%5D%20AND%20in%20vitro)]

In an effort to develop an animal model to study the biological characteristics of ^99m^Tc-anti-SSEA-1, human, rat, guinea pig, dog, rabbit, sheep, and pig polymorph nuclear leukocytes (PMN) were exposed to the labeled mAb under in vitro conditions (9). Only the human PMNs were reported to bind the radiolabeled mAb (80 ± 5%), and PMNs from the other animal species bound only ~3% of the tracer. This indicated that the mAb had a high binding specificity for the human cells (9). On the basis of this observation, the investigators concluded that this mAb could be used only in humans.

In another study, ^99m^Tc-anti-SSEA-1 mAb was shown to have a K_d_ of 1.6 × 10−^11^ M for human neutrophils and could bind to 5.1 × 10^5^ antigenic sites on these cells (9).

## Animal Studies

### Rodents

[PubMed (http://www.ncbi.nlm.nih.gov/pubmed?term=99mTc-fanolesomab%20rodentia&cmd=DetailsSearch)]

No publication is currently available.

### Other Non-Primate Mammals

[PubMed (http://www.ncbi.nlm.nih.gov/pubmed?term=99mTc-fanolesomab%20Other%20Non-Primate%20Mammals&cmd=DetailsSearch)]

No publication is currently available.

### Non-Human Primates

[PubMed (http://www.ncbi.nlm.nih.gov/pubmed?term=99mTc-fanolesomab%20Non-Human%20Primates&cmd=DetailsSearch)]

No publication is currently available.

## Human Studies

[PubMed (http://www.ncbi.nlm.nih.gov/pubmed?term=99mTc-fanolesomab%20Human%20Studies&cmd=DetailsSearch)]

Twelve patients with clinically confirmed inflammation were intravenously injected with ^99m^Tc-anti-SSEA-1 mAb, and serial anterior and posterior spot-views and whole-body single-photon emission computed tomography (SPECT) scans were acquired for all patients up to 3 h postinjection (p.i.) (8). Infections (perforated appendicitis, osteomyelitis, abscess, and inflammation) were visible in all the patients within 3 h p.i., and 11 of these infections were confirmed with other modalities. Biodistribution of the tracer in the patients was determined as described elsewhere (8). Radioactivity accumulated in each organ was presented as a percentage of the geometric mean of the total body counts. The highest uptake of radioactivity was observed in the liver (49.9 ± 3.2%), followed by the spleen (7.7 ± 0.1%), kidneys (2.4 ± 0.03%), and the bladder (1.3 ± 0.4%). At 3 h p.i., the amount of label bound to the PMNs of the patients varied from 15% to 51%, and the amount of label in the whole blood was <25% at this time point.

Tronco et al. reported that SPECT imaging with ^99m^Tc-fanolesomab at 18–30 h p.i. can be used to detect prosthetic vascular graft infection with 95% accuracy (7).

A recent report describes the use of ^99m^Tc-fanolesomab with SPECT for the imaging of five patients exhibiting renal allograft complications (10). It is pertinent to mention that it is assumed this study is published now, but it was performed before ^99m^Tc-fanolesomab was withdrawn for marketing in the United States. Two patients had very high uptake in the transplant kidney compared to the lower lumbar spine (used as control tissue for this study), and the patients were determined to have pyelonephritis (http://kidney.niddk.nih.gov/kudiseases/pubs/pyelonephritis/). One individual who had acute renal failure due to secondary humoral rejection showed a similar accumulation of the tracer in the transplant kidney and the lower lumbar spine. One patient showed a high level of radioactivity in the pelvis of the transplant kidney, indicating normal excretion of the free ^99m^Tc-pertechnetate by the organ. Another patient, who was off immunosuppressive therapy and on maintenance hemodialysis for 4 months, had an uptake of the label that was comparable to the lumbar spine, indicating there was chronic rejection of the transplant kidney in this individual. From this study, the investigators concluded that SPECT scans with ^99m^Tc-fanolesomab can probably be used to distinguish a normal functioning allograft kidney from an infected or a rejected transplant kidney. However, they caution that this procedure will have to be evaluated in a large number of patients, including a large control group, before it can be used as a diagnostic technique in the clinics.

## Supplemental Information

[Disclaimers]

No supplemental information is currently available.

## NIH Support

## References

1 Shanthly N., Aruva M.R., Zhang K., Mathew B., Thakur M.L. (2006). 99mTc-Fanolesomab: affinity, pharmacokinetics and preliminary evaluation. Q J Nucl Med Mol Imaging.
2 Love C., Tronco G.G., Palestro C.J. (2006). Imaging of infection and inflammation with 99mTc-Fanolesomab. Q J Nucl Med Mol Imaging.
3 Melendez-Alafort L., Nadali A., Pasut G., Zangoni E., De Caro R., Cariolato L., Giron M.C., Castagliuolo I., Veronese F.M., Mazzi U. (2009). Detection of sites of infection in mice using 99mTc-labeled PN(2)S-PEG conjugated to UBI and 99mTc-UBI: a comparative biodistribution study. Nucl Med Biol.
4 Chopra, A., Acetyl-lys-lys-lys-lys-lys-cys-gly-cys-gly-gly-pro-leu-tyr-lys-lys-ile-ile-lys-lys-leu-leu-glu-ser-heparin-[99mTc] (P483H-99mTc). Molecular Imaging and Contrast agent Database (MICAD) [database online]. National Library of Medicine, NCBI, Bethesda, MD, USA. Available from www.micad.nih.gov, 2004 -to current.
5 Chopra, A., 99mTc]-Acetyl-arg-arg-arg-arg-arg-cys-gly-cys-gly-gly-pro-leu-tyr-arg-arg-ile-ile-arg-arg-leu-leu-glu-ser-dermatan sulfate (99mTc-P1827DS). Molecular Imaging and Contrast agent Database (MICAD) [database online]. National Library of Medicine, NCBI, Bethesda, MD, USA. Available from www.micad.nih.gov, 2004 -to current.
6 Quigley A.M., Gnanasegaran G., Buscombe J.R., Hilson A.J. (2008). Technetium-99m-labelled sulesomab (LeukoScan) in the evaluation of soft tissue infections. Med Princ Pract.
7 Tronco G.G., Love C., Rini J.N., Yu A.K., Bhargava K.K., Nichols K.J., Pugliese P.V., Palestro C.J. (2007). Diagnosing prosthetic vascular graft infection with the antigranulocyte antibody 99mTc-fanolesomab. Nucl Med Commun.
8 Thakur M.L., Marcus C.S., Henneman P., Butler J., Sinow R., Diggles L., Minami C., Mason G., Klein S., Rhodes B. (1996). Imaging inflammatory diseases with neutrophil-specific technetium-99m-labeled monoclonal antibody anti-SSEA-1. J Nucl Med.
9 Thakur M.L., Richard M.D., White F.W. (1988). Monoclonal antibodies as agents for selective radiolabeling of human neutrophils. J Nucl Med.
10 Aygen M., Amirmokri P., Berk F., Nguyen N., Bastani B., Civelek A.C. (2011). A preliminary report on 99mTc-fanolesomab imaging of renal allograft. Nucl Med Commun.